# Alexa 680 conjugated to bovine serum albumin

Chemical name: | Alexa 680 conjugated to bovine serum albumin
Abbreviated name: | Alexa680-BSA
Synonym:
Agent Category: | Protein
Target: | Lymphatic system
Target Category: | Others
Method of detection: | Optical imaging (near-infrared fluorescence (NIRF) imaging)
Source of signal / contrast: | Alexa 680
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Lymphatic%20system&cmd=DetailsSearch)]

The lymphatic system collects lymph, the excess protein-rich fluid that diffuses out of blood vessels, and returns it to blood circulation (1). The flow of lymph in the system is unidirectional, and in addition to proteins it carries various antigens and antigen-presenting cells (activated) to the lymph nodes, which is where the effector cell and humoral immune responses are launched into the circulatory system (for details, see Alitalo (1)). A damaged lymphatic system (due to hereditary or accidental reasons) can lead to the development of a suboptimal immune response and/or lymphedema (http://www.webmd.com/a-to-z-guides/lymphedema-topic-overview) due to the accumulation of lymph, fat, and connective tissues at the affected site. There is currently no effective treatment for lymphedema (2). In addition, the functioning of the lymphatic system and the process of lymph flow are not well understood because there is a lack of suitable invasive or noninvasive method(s) (such as imaging) that can be used for the preclinical or clinical study of these physiological processes (1, 2). Quantitative lymphoscintigraphy is commonly used to visualize lymphatic function and lymph flow in animals and humans; however, the main disadvantages of using this method are the application of radioactive materials, limited spatial resolution of the images, and the possibility of direct radionuclide diffusion into the surrounding normal tissues through microcapillaries as a result of proteolysis, dissociation of radiotracer from the imaging agent, and vascular transport (3). Optical imaging has been used to assess the lymphatic functions in mice after direct intradermal injection of indocyanine green (ICG), a small molecule near-infrared fluorescence dye, but quantification of lymph flow in the animals was difficult because the dye was cleared rapidly from the interstitium by the lymphatics and blood circulation in the animals (2, 4). In another study, liposome-enclosed ICG (LP-ICG) was used for the imaging of the mouse lymphatic system, and in the same study the preparation was shown to be unstable in 50% fetal bovine serum (5). This indicated that release of free ICG into the system from the LP-ICG preparation could result in an inaccurate estimation of lymph flow in the animals. In addition, free ICG was reported to alter contractility of the rat lymphatic vessels in a dose- and dilution-dependent manner, suggesting that measurement of lymph flow with ICG may not be a true representation of the process in the animals (6).

In a continued effort to develop an agent that can be used with a noninvasive technique to measure the lymph flow in rodents, Alexa 680–labeled bovine serum albumin (Alexa680-BSA) was synthesized and evaluated with near-infrared fluorescence imaging in normal mice and rats and in lymphedema (Chy) mice (2).

### Related Resource Links

Alexa Fluor–related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books?term=Alexa%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D&cmd=DetailsSearch)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=lymphatic+system) related to lymphatic system

Lymph system (http://www.nlm.nih.gov/medlineplus/ency/article/002247.htm) (MedlinePlus, National Library of Medicine, NIH)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Alexa680-albumin%20synthesis&cmd=DetailsSearch)]

The synthesis of Alexa680-BSA has been described by Karlsen et al. (2). The conjugated albumin was purified with size-exclusion chromatography and stored as a solution (formulation not reported) with a protein concentration of 1 mg/mL at −20°C until required. The fluorescent dye/protein ratio was reported to be 2.7. The fluorescent dye–conjugated BSA was reported to have a purity of >99% as determined with high-performance liquid chromatography (HPLC).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Alexa680-albumin%20in%20vitro%20studies&cmd=DetailsSearch)]

HPLC analysis showed that Alexa680-BSA was stable for at least 3 months at 4°C (2). The Alexa680-BSA conjugate was reported to remain stable in mouse interstitial fluid or 100% mouse serum for up to 96 h at 37°C, and no free dye was detected in the preparation at the end of the incubation period (2).

Using an in vitro phantom system, a direct correlation between the concentration of Alexa680-BSA and fluorescence signal intensity was observed by Karlsen et al. (R^2^ = 0.9601) (2).

An in vitro time-domain imaging study (lifetime analysis) showed that in a solution there was a linear correlation (R^2^ = 0.9529) between the fluorescence lifetime and the albumin conjugate/free dye ratio in solution (2). This indicated that the lifetime analysis could be used to discriminate between the intact Alexa680-BSA conjugate in solution and a conjugate/free dye mixture in solution.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Alexa680-albumin%20rodentia&cmd=DetailsSearch)]

It has been shown that there was a linear correlation between the amount of Alexa680-BSA injected into the mouse paw skin (~15–90 pmol) and the intensity of the fluorescent signal (R^2^ = 0.9232) obtained from the site of injection (2).

A lifetime analysis of the fluorescence signal generated by the probe injected into the hind limbs of C57BL/6 mice (n = 4 animals/group) from 1 h to 6 h postinjection (p.i.) showed that the average lifetime of the signal was 1.61 ± 0.01 ns at each time point (2). Without blood or lymph circulation, any dye that has dissociated from the probe would accumulate in the skin of dead animals. Therefore, euthanized mice were injected with the fluorescent probe as described above, and the average lifetime of the signal at each time point was determined. The lifetime of the signal from the euthanized animals was reported to be 1.61 ± 0.0005 ns. Because the fluorescence lifetime of the signal in the live and euthanized animals was identical, the investigators concluded that the conjugate was not degraded in vivo and was probably suitable to investigate the flow of lymph in rodents (2).

To investigate the lymphatic clearance of Alexa680-BSA in C3H and C57BL/6 mice (n = 6 animals/time point per strain), the rodents were given an intradermal injection of the tracer in the hind leg paw skin (2). The rodents were imaged every 1 h for a total of 6 h, and the dye removal rate constant, k, that defines the lymph flow was calculated from the images as explained by Karlsen et al. (2). The fluorescent conjugate was removed from the injection site significantly faster (P = 0.01) in the C57BL/6 mice (k = −0.40 ± 0.03%/min) than in the C3H mice (k = −0.30 ± 0.02%/min). These observations indicated that the lymph flow in the animals was strain-dependent.

In another study, the investigators studied the effect of local vasoconstriction on the lymph flow in C57BL/6 mice (2). The animals were given an intradermal injection of the probe in the paw, and 1 h later the mice were injected with endothelin-1 (ET-1; a potent vasoconstrictor; 100 pmol) at a site close to the probe injection site to induce local vasoconstriction. Control animals received an injection of normal saline. At 60 min after the ET-1 injection, the average k value for the probe injection site was −0.04 ± 0.03%/min, which was significantly less (P = 0.001) than the value in the control animals (−0.22 ± 0.03%/min). After the initial inhibition of clearance of the probe at the site of the ET-1 injection, the clearance of Alexa680-BSA was shown to be restored to control levels for at least 1 h (k values were −0.25 ± 0.02%/min and −0.23 ± 0.03%/min for the ET-1 and the control mice, respectively) (2).

The effect of overhydration on lymph flow was investigated in anesthetized Sprague-Dawley rats (2). The animals were injected intradermally with Alexa680-BSA on the right hind limb paw. The experimental rats (n = 6 animals) had their kidneys ligated to prevent water excretion, and these animals were intravenously infused with isotonic saline (15% of body weight) to facilitate volume expansion. Control animals (n = 5 rats; anesthetized) were not subject to surgery or infused with saline. The paw was scanned every 30 min; from the images the average k value for the control rats was calculated to be −0.09 ± 0.07%/min compared with a significantly higher value of −0.37 ± 0.06%/min for the experimental animals (P = 0.012; approximately four-fold higher). These observations indicated that the fluorescent conjugate was cleared rapidly from the injection site in the test rats. This showed that Alexa680-BSA could also be used to measure changes in lymph flow in these rodents.

Chy lymphedema mice lack lymphatics in the dermis of the paw, but have a normal lymphatic system in the skeletal muscle of the hind limbs (2). The washout of Alexa680-BSA from the paw skin and thigh muscle of the Chy mice (n = 6 animals) was studied by acquiring images over a 6-h period. As a control, the washout of the probe was similarly studied in normal C3H mice (n = 6 animals). The k value averaged −0.16 ± 0.01%/min in the paw skin of the Chy mice, which was significantly lower (P < 0.001) than the k from the paw skin of the C3H mice (−0.30 ± 0.02%/min). The k values from the hind limb muscle of the Chy and C3H mice were −0.28 ± 0.03%/min (n = 7 animals) and −0.32 ± 0.02%/min (n = 6 animals), respectively.

From these studies, the investigators concluded that Alexa680-BSA can be used to study the lymph flow in rodents (2).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Alexa680-albumin%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Alexa680-albumin%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Alexa680-albumin%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Alitalo K. (2011). The lymphatic vasculature in disease. Nat Med.
2 Karlsen T.V., McCormack E., Mujic M., Tenstad O., Wiig H. (2012). Minimally invasive quantification of lymph flow in mice and rats by imaging depot clearance of near-infrared albumin. Am J Physiol Heart Circ Physiol.
3 Modi S., Stanton A.W., Mortimer P.S., Levick J.R. (2007). Clinical assessment of human lymph flow using removal rate constants of interstitial macromolecules: a critical review of lymphoscintigraphy. Lymphat Res Biol.
4 Kwon S., Sevick-Muraca E.M. (2007). Noninvasive quantitative imaging of lymph function in mice. Lymphat Res Biol.
5 Proulx S.T., Luciani P., Derzsi S., Rinderknecht M., Mumprecht V., Leroux J.C., Detmar M. (2010). Quantitative imaging of lymphatic function with liposomal indocyanine green. Cancer Res.
6 Gashev A.A., Nagai T., Bridenbaugh E.A. (2010). Indocyanine green and lymphatic imaging: current problems. Lymphat Res Biol.